# Bovine serum albumin–stabilized gold nanoclusters conjugated with folate and indocyanine green derivative 02

Chemical name: | Bovine serum albumin–stabilized gold nanoclusters conjugated with folate and indocyanine green derivative 02
Abbreviated name: | Au-FA-MPA
Synonym: | Au-BSA-FA-MPA, Au-BSA-FA-ICG-Der-02, Au-FA-ICG-Der-02
Agent category: | Compound
Target: | Folate receptor
Target category: | Receptor
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | ICG-Der-02 (MPA)
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Au-FA-MPA)]

Folic acid (FA) is a water-soluble B vitamin (1). It is essential for methylation and DNA synthesis. The primary pathway for entry of folate into cells is via a facilitated transporter, which has a low affinity for folate (K_m_, 1–5 μM). Some cells in the choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a higher-affinity receptor (K_d_, 0.5 nM) that allows folate uptake via receptor-mediated endocytosis. Some human epithelial tumor cells were found to overexpress folate receptors (2). More than 90% of human ovarian and endometrial cancers express the high-affinity receptor, which is absent in normal tissues. Breast, colorectal, renal, and lung carcinomas also overexpress the high-affinity folate receptor but to a lesser frequency (20%–50%).

Among the various optical imaging agents, only indocyanine green (ICG (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=15096)), with NIR fluorescence absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment (3-6). It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications, such as optical imaging and mapping of both the lymphatic vessels and lymph nodes in cancer patients for surgical dissection of tumor cells and endoscopic imaging of the pancreas and colon. Gold (Au) nanoclusters (NCs) are comprised of a few tens of Au atoms that possess the ability to emit strong fluorescence, of which the wavelength is tunable in the range of the visible to near-infrared spectral region (7). Chen et al. (8) prepared bovine serum albumin–stabilized Au NCs (Au-BSA) for conjugation with biomolecules for specific targeting and with near-infrared dye for optical imaging. Folate was conjugated to the amino groups of BSA. The ICG derivative 02 (ICG-Der-02, also known as MPA) contains one carboxyl functional group for covalent conjugation to the amino groups of BSA on the surface of Au-BSA NCs. MPA is a hydrophilic dye. Chen et al. (9) evaluated Au-BSA-FA-MPA (Au-FA-MPA) for in vivo NIR optical imaging of folate receptor expression in tumor-bearing mice.

### Related Resource Links:

- Chapters in MICAD (folate receptor (http://www.ncbi.nlm.nih.gov/books?term=folate%20receptor%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D), ICG (http://www.ncbi.nlm.nih.gov/books?term=ICG%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (folate receptor (http://www.ncbi.nlm.nih.gov/gene/2348))
- Articles in Online Mendelian Inheritance in Man (OMIM) (folate receptor (http://www.ncbi.nlm.nih.gov/omim/136430))
- Clinical trials (folate receptor (http://www.clinicaltrials.gov/ct2/results?term=folate+receptor), ICG (http://www.clinicaltrials.gov/ct2/results?term=ICG))
- Drug information in FDA (folate receptor (http://google2.fda.gov/search?q=folate+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15), ICG (http://google2.fda.gov/search?q=Indocyanine+Green&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=4&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Au-FA-MPA%20and%20synthesis)]

Au-BSA NCs were prepared by addition of HAuCl_4_ solution (10 mM) to BSA solution (50 mg/ml) under vigorous stirring for 30 min at 37°C (9). The mixture was stirred for an additional 12 h at 37°C. FA was activated with N,N'-dicyclohexylcarbodiimide (DDC) and N-hydroxysuccinimide (NHS) (molar ratio of FA:DCC:NHS was 1:1.5:2) in dimethyl sulfoxide for 12 h at 50°C. The activated FA was extracted with acetone. MPA (1.0 mg) was activated with DDC and NHS (molar ratio of MPA:DCC:NHS was 1:1.5:2) for 3 h at room temperature. The activated FA and Au-BSA were mixed in Tris buffer (pH 8) for 12 h at 4°C. Au-BSA-FA NCs were isolated with column chromatography. The activated MPA was incubated with AU-BSA-FA NCs for 12 h at room temperature. The final product, Au--FA-MPA, was isolated with column chromatography. The mean hydrodynamic diameter of Au-BSA (measured with laser particle size analysis) was 3.74 nm (polydispersity = 0.373), whereas Au-FA-MPA exhibited a relatively larger diameter of 4.82 nm (polydispersity = 0.453), indicating the successful addition of FA and MPA molecules. The absorption spectra of FA, Au-BSA, MPA, Au-BSA-FA, and Au-FA-MPA exhibited absorbance peaks at 365, 232, and 780 nm, which corresponded to FA, Au, and MPA, respectively. The number of Au, BSA, FA, and MPA moieties per Au-FA-MPA was not reported. Au-FA-MPA displayed spectral properties similar to those of MPA, with maximum absorption at 780 nm and maximum emission at 810 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Au-FA-MPA%20and%20in%20vitro)]

The cytotoxic effects of Au-BSA and Au-FA-MPA (0.01–1,000 µM) were assessed in human cell lines HepG-2 (liver cancer) and MDA-MB-231 (breast cancer) for 24 h at 37°C (9). Approximately 95% viability was observed with 0.01–1 µM, with 85% at 1 mM. Confocal fluorescence microscopy analysis showed little binding of Au-BSA and Au-FA-MPA to HepG-2 cells (low folate receptor expression), whereas strong fluorescence signal (MPA) was observed around the nuclei of MCF-7 cells (high folate receptor expression) with Au-FA-MPA but not with Au-BSA-MPA. No blocking studies were performed with excess FA.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Au-FA-MPA%20and%20rodentia)]

Chen et al. (9) performed in vivo whole-body NIR fluorescence imaging studies in nude mice (n = 5/group) bearing MDA-MB-231 human breast cancer (high folate receptor expression), HTC116 human colon cancer (moderate to high folate receptor expression) or HepG-2 human lung cancer xenografts (low folate receptor expression) at 0.5–96 h after intravenous injection of Au-FA-MPA (10 mg/kg body weight). Images showed that NIR fluorescence (MPA) spread all over the body at 0.5 h and then concentrated in the liver and kidney. Most NIR fluorescence of the normal tissues was cleared from the body by 10 h. MDA-MB-231 tumors were clearly visualized at 2 h, and the NIR fluorescence peaked at 20 h. The tumor NIR fluorescence was still detectable at 96 h. HTC116 tumors exhibited weaker NIR fluorescence than the MDA-MB-231 tumors at 2–4 h, and fluorescence was almost indistinguishable from the background by 20 h. On the other hand, HepG-2 tumors showed a low fluorescence signal at 3 h, which became undetectable by 10 h. Tumor/background ratios for MDA-MB-231 tumors were 2.9 ± 0.5 at 1 h, 11.4 ± 0.6 at 20 h, and 6.4 ± 0.2 at 72 h. Tumor/background ratios for HTC116 tumors were 2.1 ± 0.4 at 1 h, 6.4 ± 0.6 at 10 h, and 2.2 ± 0.3 at 48 h. Tumor/background ratios for HepG-2 tumors were 3.8 ± 0.5 at 3 h and 1.2 ± 0.1 at 20 h. Ex vivo NIR fluorescence images of the excised tumors and normal organs at 5 h showed strong signals in the MDA-MB-231 tumor, HTC116 tumor, liver, and kidney but weak signal in the HepG-2 tumor. The excised organs from normal mice exhibited little histological change at 7 d after injection of Au-FA-MPA (250 mg/kg). No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Au-FA-MPA%20and%20%28pig%20or%20dog%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Au-FA-MPA%20AND%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Au-FA-MPA%20and%20human)]

No publication is currently available.

## References

1 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
2 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
3 Yannuzzi, L.A., Indocyanine green angiography: a perspective on use in the clinical setting. Am J Ophthalmol, 2011151(5): p. 745-751 e1.
4 Yamamoto M., Sasaguri S., Sato T. (2011). Assessing intraoperative blood flow in cardiovascular surgery. Surg Today.
5 Schaafsma B.E., Mieog J.S., Hutteman M., van der Vorst J.R., Kuppen P.J., Lowik C.W., Frangioni J.V., van de Velde C.J., Vahrmeijer A.L. (2011). The clinical use of indocyanine green as a near-infrared fluorescent contrast agent for image-guided oncologic surgery. J Surg Oncol.
6 Manizate F., Hiotis S.P., Labow D., Roayaie S., Schwartz M. (2010). Liver functional reserve estimation: state of the art and relevance for local treatments: the Western perspective. J Hepatobiliary Pancreat Sci.
7 Huang C.C., Chen C.T., Shiang Y.C., Lin Z.H., Chang H.T. (2009). Synthesis of fluorescent carbohydrate-protected Au nanodots for detection of Concanavalin A and Escherichia coli. Anal Chem.
8 Chen H., Li B., Ren X., Li S., Ma Y., Cui S., Gu Y. (2012). Multifunctional near-infrared-emitting nano-conjugates based on gold clusters for tumor imaging and therapy. Biomaterials.
9 Chen H., Li S., Li B., Ren X., Mahounga D.M., Cui S., Gu Y., Achilefu S. (2012). Folate-modified gold nanoclusters as near-infrared fluorescent probes for tumor imaging and therapy. Nanoscale.